# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-PEGylated dimeric cyclic arginine-glycine-aspartic acid peptide

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-pegylated dimeric cyclic arginine-glycine-aspartic acid peptide
Abbreviated name: | ^64^Cu-DOTA-PEG-E[c(RGDyK)]_2_
Synonym: | ^64^Cu-pegylated dimeric c(RGDyK), ^64^Cu-PEG-dimeric RGD
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | PEG is a heterofunctional polyethylene glycol with a molecular weight of 3,400. Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov). Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu-DOTA-PEG-E%5Bc(RGDyK)%5D2+OR+(64Cu-labeled+PEGylated+dimeric+RGD+peptide)&WebEnv=0EbqbPa6NqNIEwbMZezc6lbKUXIdBOtM3mIEWg3Y1WWecZismpSuB03NndBvvvVo3T0wxJp9_EWd2s%40D47B4E116601962)]

^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid –PEGylated dimeric cyclic arginine-glycine-aspartic acid peptide {^64^Cu-DOTA-PEG-E[c(RGDyK)]_2_} is an integrin-targeted molecular imaging agent developed for positron emission tomography (PET) of tumor vasculature and tumor angiogenesis (1). ^64^Cu is a positron emitter with a physical half-life (t_½_) of 12.8 h.

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiologic processes (2, 3). Among the molecules that regulate angiogenesis are integrins, which comprise a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5). These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Expression of integrin α_v_β_3_ receptors on endothelial cells is stimulated by angiogenic factors and environments. The integrin α_v_β_3_ receptor is generally not found in normal tissue, but it is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature (1).

Molecular imaging probes carrying the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (6, 7). Various RGD peptides in both linear and cyclic forms (RGDfK or RGDyK) have been developed for in vivo binding to integrin α_v_β_3_ (8). It has been hypothesized that cyclic RGD peptide may have a faster rate of receptor binding or a slower rate of dissociation from the integrin α_v_β_3_ than linear single RGD peptides (9). They also suggested that the increase in molecular size might prolong circulation time and reduce tumor washout rate. Chen et al. (10) prepared a cyclic RGD D-Tyr analog [^64^Cu-DOTA-c(RGDyK)] and showed the cyclic peptide had prolonged tumor radioactivity retention but persistent liver radioactivity. To improve the pharmacokinetics and tumor retention of the radiolabeled peptide, Chen et al. (11) modified c(RGDyK) with monofunctional methoxy-polyethylene glycol (mPEG; molecular weight = 2,000) and showed that the modified PEGylated RGD peptide had faster blood clearance, lower kidney uptake, and prolonged tumor uptake. Using the same strategy, Chen et al. (12) inserted a heterobifunctional PEG linker (molecular weight = 3,400) between DOTA and c(RGDyK) to produce ^64^Cu-DOTA-PEG-c(RGDyK). The PEG moiety appeared to improve the in vivo kinetics of this PET radioligand. Chen et al. (13) also observed that a dimeric RGD peptide E[c(RGDyK)]_2_ had higher binding affinity than the monomeric analog. Subsequently, the same research group also reported the successful use of a heterobifunctional PEG to prepare ^64^Cu-lableled PEGylated E[c(RGDyK)]_2_ peptide (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu-DOTA-PEG-E%5Bc(RGDyK)%5D2+OR+(64Cu-labeled+PEGylated+dimeric+RGD+peptide))+AND+synthesis&WebEnv=0rVuNvNUw0g5mUYm89kzT5AB4gzCIaV2PAbedR3sL9mv4SBZaKKvdDKqbBJVGgjiBa5LiLD82IeHLb%254)]

Chen et al. (1) reported the synthesis of ^64^Cu-DOTA-PEG-E[c(RGDyK)]_2_. The E[c(RGDyK)]_2_ peptide was prepared by coupling Boc-Glu-OH with two equivalents of monomeric RGD peptide followed by trifluoroacetic acid (TFA) cleavage. The monomeric c(RGDyK) was first prepared via solution cyclization of the fully protected linear pentapeptide H-Gly-Asp(OtBu)-D-Tyr(OtBu)-Lys(Boc)-Arg(Pbf)-OH, followed by TFA deprotection in the presence of the free radical scavenger triisopropylsilane. A bifunctional PEG (molecular weight 3,400) was used. The DOTA-PEG-E[c(RGDyK)]_2_ conjugate was prepared from t-butoxycarbonyl (t-Boc)-NH-PEG-E[c(RGDyK)]_2_ which was synthesized by reacting t-Boc-protected PEG succinimidyl ester with the E[c(RGDyK)]_2_ peptide in 0.2 M Na_2_B_4_O_7_ buffer (pH 8.3) overnight at 4ºC. The t-Boc-NH-PEG-E[c(RGDyK)]_2_ was then dissolved in 95% TFA at room temperature for 2 h to produce the NH_2_-PEG-E[c(RGDyK)]_2_ conjugate. DOTA was obtained commercially. The DOTA-PEG-c(RGDyk) conjugate was prepared by activating DOTA in situ by 1-ethyl-3-[3-(dimethylamino)propyl]carbodiimide (EDC) and N-hydroxysulfonosuccinimide (SNHS) in a molar ratio of 10:5:4 (DOTA:EDC:SNHS).The NH_2_-PEG-E[c(RGDyk)]_2_ conjugate in water at 4ºC was added to the resultant DOTA-sulfosuccinimydyl ester (OSSu), and the pH was adjusted to 8.5. The reaction mixture was allowed to incubate overnight at 4ºC. The final product DOTA-PEG-E[c(RGDyk)]_2_ conjugate was then purified by semi-preparative high-performance liquid chromatography (HPLC) with a final yield of ~60%. The molecular weight of the DOTA-PEG-E[c(RGDyk)]_2_ conjugate was determined to be 5,100 by matrix-assisted desorption/ionization time-of-flight mass spectroscopy and appeared to agree with the theoretical value. The purified product was labeled with ^64^Cu by addition of ^64^Cu chloride in the ratio of 25 μg peptide per 5 MBq (0.135 mCi) ^64^Cu in 0.1 N sodium acetate (pH 5.5) buffer. This was followed by incubation at 50ºC for 50 minutes. The reaction was terminated by addition of ethylenediaminetetraacetic acid. ^64^Cu-DOTA-PEG-E[c(RGDyK)]_2_ was purified with a C-18 Sep-Pak cartridge using 85% ethanol as the elution solvent. The radiochemical yield was >95%. After Sep-Pak purification, the radiochemical purity was >99%. The specific activity of ^64^Cu-DOTA-PEG-E[c(RGDyK)]_2_ was ~18,500 GBq/mmol (500 Ci/mmol, decay-corrected).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20in%20vitro)]

Competitive binding experiments of unlabeled DOTA-PEG-E[c(RGDyK)]_2_ for integrin α_v_β_3_ on the surface of NSCLC NCI-H1975 human female lung adenocarcinoma cells were conducted by the use of ^125^I-echistatin as a radioligand (1). The 50% inhibitory concentration (IC_50_) of DOTA-PEG-E[c(RGDyK)]_2_ was 84.9 nM. In comparison, the IC_50_ for unpegylated E[c(RGDyK)]_2_ was 11.1 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu-DOTA-PEG-E%5Bc(RGDyK)%5D2+OR+(64Cu-labeled+PEGylated+dimeric+RGD+peptide))+AND+rodentia&WebEnv=04mJ0lNEot-6VhOcuJeX9W91eFfAZfKfkibUGSw-bMu4vtMB0e2dlT-Fq_5M7OGl9JanM0NFJkWQ-b%40)]

Biodistribution studies of ^64^Cu-DOTA-PEG-E[c(RGDyK)]_2_ were conducted in severe combined immunodeficient (SCID-bg) mice bearing s.c. NCI-H1975 (1). Each mouse received 370 kBq (10 μCi) of ^64^Cu-DOTA-PEG-E[c(RGDyK)]_2_ by i.v. administration. The radioligand was rapidly cleared from the blood. The radioactivity levels (n = 3) in percent dose per g (% ID/g) in the tumor were 1.87 ± 0.05 (0.5 h), 2.64 ± 0.14 (1 h), 1.35 ± 0.06 (2 h), 1.46 ± 0.12 (4 h), and 1.15 ± 0.07 (24 h). The radioactivity levels in the blood were 0.57 ± 0.19 (0.5 h), 0.17 ± 0.02 (1 h), 0.05 ± 0.01 (2 h), 0.04 ± 0.02 (4 h), and 0.04 ± 0.01 (24 h). The tumor/blood ratios were 3.58 ± 1.43 (0.5 h), 15.3 ± 1.06 (1 h), 27.9 ± 6.37 (2 h), 36.9 ± 13.1 (4 h), and 28.7 ± 3.71 (24 h). The radioligand was primarily excreted by the kidneys. The radioactivity levels in the kidney were 3.50 ± 0.54 (0.5 h), 1.92 ± 0.26 (1 h), 1.63 ± 0.04 (2 h), 1.61 ± 0.17 (4 h), and 1.15 ± 0.11 (24 h). Both liver and lung radioactivity levels were relatively low. There was minimal radioactivity in other organs. With coinjection of 10 mg/kg unlabeled c(RGDyK) peptide, the tumor radioactivity was decreased by four times to 0.68 ± 0.10 at 1 h. When compared to the unpegylated radioligand, the authors suggested that the pegylated radioligand had a relatively more rapid renal clearance and a lower liver accumulation. However, the tumor radioactivity was also lowered because the pegylated peptide had a lower receptor binding affinity than the unpegylated peptide.

Imaging of 11.1 MBq (300 μCi) ^64^Cu-DOTA-PEG--E[c(RGDyK)]_2_ with microPET was conducted in SCID-bg mice bearing the s.c. tumors (1). In addition, orthotopic lung cancer tumors (NCI-H1975 cells injected directly into the upper lung lobe) and its metastases were also induced in the same mice. At 2 h after injection, PET imaging clearly visualized the s.c. tumor, the primary orthotopic lung tumor and its metastases to the contralateral lung, mediastinum, and diapghragm. The kidneys, liver and urinary bladder were also visible on the image. In comparison, a [^18^F]FDG scan on the same mouse visualized the primary lung cancer but failed to visualize the metastases because of the high cardiac and lung radioactivity background. Whole-body autoradiography of the mice after PET imaging showed a distribution pattern similar to those of the biodistribution and imaging studies. Chen et al. (1) concluded that ^64^Cu-DOTA-PEG--E[c(RGDyK)]_2_ had similar blood clearance, more rapid renal clearance, reduced hepatic uptake, but also lower tumor uptake when compared with the unpegylated peptide.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu-DOTA-PEG-E%5Bc(R(GDyK)%5D2+OR+(64Cu-labeled+PEGylated+dimeric+RGD+peptide))+AND+(dog+OR+rabbit+OR+pig+OR+sheep)&WebEnv=0yBfP-_5oHMbPRCcXrFExnTCxMVXZdDIwMDMLGmUzKsIbPe8yTDSnKpNL)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu-DOTA-PEG-E%5Bc(R(GDyK)%5D2+OR+(64Cu-labeled+PEGylated+dimeric+RGD+peptide))+AND+(primate+NOT+human)&WebEnv=0FhD1fAarVCOSuwWGU4UGBEuxkoFazsj33sn2EqvHEd379drG6yKf2VFOrbqgB1q4KE3H)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu-DOTA-PEG-E%5BAll+Fields%5D+AND+(64Cu-labeled%5BAll+Fields%5D+AND+PEGylated%5BAll+Fields%5D+AND+dimeric%5BAll+Fields%5D+AND+(%22arginyl-glycyl-aspartic+acid%22%5BSubstance+Name%255)]

No publication is currently available.

## NIH Support

NIBIB R21 EB001785, NCI P20 CA86532.

## References

1 Chen X., Sievers E., Hou Y., Park R., Tohme M., Bart R., Bremner R., Bading J.R., Conti P.S. (2005). Integrin alpha v beta 3-targeted imaging of lung cancer. Neoplasia.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Paulhe F., Manenti S., Ysebaert L., Betous R., Sultan P., Racaud-Sultan C. (2005). Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des.
4 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
5 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
6 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
7 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
9 Wu Y., Zhang X., Xiong Z., Cheng Z., Fisher D.R., Liu S., Gambhir S.S., Chen X. (2005). microPET imaging of glioma integrin {alpha}v{beta}3 expression using (64)Cu-labeled tetrameric RGD peptide. J Nucl Med.
10 Chen X., Park R., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). MicroPET and autoradiographic imaging of breast cancer alpha v-integrin expression using 18F- and 64Cu-labeled RGD peptide. Bioconjug Chem.
11 Chen X., Park R., Shahinian A.H., Bading J.R., Conti P.S. (2004). Pharmacokinetics and tumor retention of 125I-labeled RGD peptide are improved by PEGylation. Nucl Med Biol.
12 Chen X., Hou Y., Tohme M., Park R., Khankaldyyan V., Gonzales-Gomez I., Bading J.R., Laug W.E., Conti P.S. (2004). Pegylated Arg-Gly-Asp peptide: 64Cu labeling and PET imaging of brain tumor alphavbeta3-integrin expression. J Nucl Med.
13 Chen X., Liu S., Hou Y., Tohme M., Park R., Bading J.R., Conti P.S. (2004). MicroPET imaging of breast cancer alphav-integrin expression with 64Cu-labeled dimeric RGD peptides. Mol Imaging Biol.